# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-interleukin-18-binding protein-Fc

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-interleukin-18-binding protein-Fc
Abbreviated name: | ^64^Cu-DOTA-IL-18bp-Fc
Synonym:
Agent category: | Polypeptide
Target: | Interleukin-18 (IL-18)
Target category: | Acceptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=89111129) and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=10068) for more information about the IL-18bp.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp)]

Interleukin-18 (IL-18) is a proinflammatory cytokine produced by macrophages and activated T cells (1, 2), and it plays an important role in inflammation and immune response (3, 4). A variety of normal and malignant cells can produce and respond to IL-18 through its receptor (IL-18R). A soluble secreted IL-18 binding protein (IL-18bp) was found to bind to IL-18 with high affinity (dissociation constant (K_d_) = 0.4 nM) and neutralize the biological effects of IL-18 by blocking its interaction with IL-18R (5, 6). IL-18bp is a 40-kDa glycoprotein with an immunoglobulin (Ig) domain. Cao et al. (7) constructed a divalent IL-18bp-Fc fusion protein by joining IL-18bp cDNA to the CH_2_ and CH_3_ domains of human IgG_1_ in an expression plasmid. IL-18bp-Fc binds human, mouse, and rat IL-18 with subnanomolar affinity (6). 1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) has been successfully coupled to IL-18bp-Fc and labeled with ^64^Cu to produce a molecular imaging agent with the potential to target breast cancer lung metastasis. ^64^Cu is a positron emitter with a physical half-life of 12.7 h and is suitable for positron emission tomography (PET) imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp+Cu+and+synthesis)]

Cao et al. (7) reported the synthesis of ^64^Cu-DOTA-IL-18bp-Fc. DOTA was activated by 1-ethyl-3-[3-(dimethylamino)-propyl]carbodiimide (EDC) and N-hydroxysulfonosuccimide (SNHS) (pH 5.5) for 30 min with a molar ratio of 10:5:4 (DOTA/EDC/SNHS). The DOTA-IL-18bp-Fc conjugate was purified with a PD-10 column, and the number of DOTA molecules per protein molecule was 2.5. For radiolabeling, 30 μg DOTA-IL-18bp-Fc was added to 37 MBq (1 mCi) ^64^CuCl_2_ diluted in 300 μl of 0.1 M sodium acetate buffer. The reaction mixture was incubated for 1 h at 40ºC. ^64^Cu-IL-18bp-Fc was purified with PD-10 column chromatography with a radiolabeling yield of 21%. The specific activity and radiochemical purity of ^64^Cu-DOTA-IL-18bp-Fc were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp+Cu+AND+in+vitro)]

Faggioni et al. (6) performed binding experiments with IL-18bp-Fc with the use of a Biacore sensor chip immobilized with human, mouse, or rat IL-18 with K_d_ values of 4.99, 0.33, and 1.84 nM, respectively. No binding data were reported for DOTA-IL-18bp-Fc.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp+Cu+AND+rodentia)]

Cao et al. (7) performed PET imaging studies in normal mice and mice bearing fLuc-4T1 breast cancer lung metastases (n = 3/group). Each mouse received 7.4 MBq (0.2 mCi) ^64^Cu-DOTA-IL-18bp-Fc by intravenous injection. The radioactivity levels in percent injected dose per cc (% ID/cc) were obtained at 1 h and 4 h after injection with fLuc-4T1 tumor lung uptake values of 8.3 ± 0.5% ID/cc and 10.1 ± 0.3% ID/cc, respectively. On the other hand, the lung uptake in normal mice was 2.5% ID/cc at 1 h and 1.5 ± 1.0% ID/cc at 4 h. The liver uptake was prominent in both normal and tumor mice. Biodistribution studies showed that the fLuc-4T1 tumor lung uptake was 12.0% ID/organ and 7.6% ID/organ at 4 h and 48 h, respectively. The lung uptake in normal mice was 1.5% ID/organ at 4 h. The distribution patterns for other organs were similar in normal mice and mice bearing fLuc-4T1 breast cancer lung metastases (n = 3/group). The liver (14% ID/g) showed the highest uptake, followed by the kidneys, intestines, blood, stomach, spleen, and heart with radioactivity levels of 7–10% ID/organ at 4 h. The radioactivity level in the blood declined to ~3% ID/g at 48 h, whereas the tumor lung, liver, kidneys, intestines, stomach, and heart exhibited a moderate decline at 48 h with radioactivity levels higher than the blood. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp+Cu+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp+Cu+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IL-18bp+Cu+AND+human)]

No publication is currently available.

## NIH Support

R01 CA119053, R21 CA121842, R21 CA102123, P50 CA114747, U54 CA119367, R24 CA93862

## References

1 Dinarello C.A. (1999). Interleukin-18. Methods.
2 Arend W.P., Palmer G., Gabay C. (2008). IL-1, IL-18, and IL-33 families of cytokines. Immunol Rev.
3 Dinarello C.A. (2007). Interleukin-18 and the pathogenesis of inflammatory diseases. Semin Nephrol.
4 Dinarello C.A., Fantuzzi G. (2003). Interleukin-18 and host defense against infection. J Infect Dis.
5 Dinarello C.A. (2000). Targeting interleukin 18 with interleukin 18 binding protein. Ann Rheum Dis.
6 Faggioni R., Cattley R.C., Guo J., Flores S., Brown H., Qi M., Yin S., Hill D., Scully S., Chen C., Brankow D., Lewis J., Baikalov C., Yamane H., Meng T., Martin F., Hu S., Boone T., Senaldi G. (2001). IL-18-binding protein protects against lipopolysaccharide- induced lethality and prevents the development of Fas/Fas ligand-mediated models of liver disease in mice. J Immunol.
7 Cao Q., Cai W., Niu G., He L., Chen X. (2008). Multimodality imaging of IL-18--binding protein-Fc therapy of experimental lung metastasis. Clin Cancer Res.